# Anti-vascular cell adhesion molecule monoclonal antibody M/K-2.7 conjugated cross-linked iron oxide-Cy5.5 nanoparticles

Chemical name: | Anti-vascular cell adhesion molecule monoclonal M/K-2.7 conjugated cross-linked iron oxide-Cy5.5 nanoparticles
Abbreviated name: | VCAM-NP
Synonym: | VCAM-CLIO-Cy5.5, M/K-2.7-CLIO-Cy5.5
Agent Category: | Antibody
Target: | Vascular cell adhesion molecule-1 (VCAM-1)
Target Category: | Antibody-antigen binding
Method of detection: | Magnetic resonance imaging (MRI), optical near-infrared (NIR) fluorescence
Source of signal/contrast: | Iron oxide, Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=54648638), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=46249772) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412) for more information about VCAM-1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=VCAM-1+nanoparticle)]

Optical fluorescence imaging is increasingly being used to obtain images of biological functions of specific targets in vitro and in small animals (1, 2). Near-infrared (NIR) fluorescence (700–900 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in vitro and in small animals.

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the nuclear density (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (3). Cross-linked iron oxide (CLIO) nanoparticles and other iron oxide formulations affect T2 primarily and lead to a decreased signal.

A multimodal nanoparticle probe that consists of a contrast agent and a NIR fluorochrome may provide consistent information. CLIO nanoparticles can be internalized by cells of the reticuloendothelial system and have long circulating times within an animal body. The blood half-life of CLIO is about 10 h in mice (4). The accumulation of nanoparticles in cells causes a reduction in signal intensity with T2-weighted (T2*W) spin-echo pulse sequences. NIR fluorochromes (e.g., Cy5.5) provide an improved optical (NIR) signal from tissue. CLIO-Cy5.5 has been developed as a probe for multimodality imaging (5).

Endothelial cells are important in inflammatory responses (6, 7). Bacterial lipopolysaccharide (LPS), virus, inflammation, and tissue injury increase tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and other cytokine and chemokine secretion. Emigration of leukocytes from blood is dependent on their ability to roll along endothelial cell surfaces and subsequently adhere to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell-surface adhesion molecules, such as intracellular adhesion molecule-1, vascular cell adhesion molecule-1 (VCAM-1), integrins, and selectins. Chemokines are chemotactic toward leukocytes and toward sites of inflammation and tissue injury. The movement of leukocytes through endothelial junctions into the extravascular space are highly orchestrated through various interactions with different adhesion molecules on endothelial cells (8).

VCAM-1 is found in very low levels on the cell surface of resting endothelial cells and other vascular cells, such as smooth muscle cells and fibroblasts (9-13). VCAM-1 binds to its counterligand, very late antigen-4 (VLA-4) integrin, on the cell surface of leukocytes. IL-1 and TNFα increase expression of VCAM-1 and other cell adhesion molecules on the vascular endothelial cells, which leads to leukocyte adhesion to the activated endothelium. Furthermore, VCAM-1 expression was also induced by oxidized low-density lipoproteins under atherogenic conditions (14). Overexpression of VCAM-1 by atherosclerotic lesions plays an important role in their progression toward vulnerable plaques, which may erode and rupture. CLIO nanoparticles targeted with anti-VCAM-1 antibody are being developed as a non-invasive agent for VCAM-1 expression in vascular endothelial cells during different stages of inflammation in atherosclerosis (15). Anti-VCAM-1 M/K-2.7 monoclonal antibody (mAb) conjugated cross-linked iron oxide-Cy5.5 nanoparticles (VCAM-CLIO-Cy5.5 or VCAM-NP) is a multimodal agent that consists of CLIO nanoparticles with attachment of M/K-2.7 mAb and Cy5.5.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+nanoparticle+synthesis)]

The synthesis of VCAM-CLIO-Cy5.5 nanoparticles was described by Tsourkas et al. (15). The amino-CLIO nanoparticles (~40 amino groups/nanoparticle, 32.5 nm in diameter; R1 = 21.5 mM^-1^s^-1^ and R2 = 54.2 mM^-1^s^-1^) were labeled with Cy5.5 using monofunctional N-hydroxysuccinimide (NHS) to form amino-CLIO-Cy5.5 nanoparticles, which were then carboxylated with NHS-COOH. Anti-VCAM-1 M/K-2.7 mAb or a control antibody was conjugated to the purified carboxylated nanoparticles using carbodiimide and sulfo-NHS to yield the multimodal VCAM-CLIO-Cy5.5 and IgG-CLIO-Cy5.5 nanoparticles, which had ~10 Cy5.5 molecules per nanoparticle and 0.87 mg (5.8 nmol) of M/K-2.7 mAb or 0.63 mg (4.2 nmol) of control antibody per mg Fe.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+nanoparticle+in+vitro)]

Tsourkas et al. (15) performed cell-binding assays with VCAM-CLIO-Cy5.5 using murine heart endothelial cells (MHEC). Using fluorescence flow cytometry, VCAM-CLIO-Cy5.5 bound to individual MHEC cells, whereas IgG-CLIO-Cy5.5 did not. A corresponding decrease in MRI signal intensity of the cell lysates was observed on a T2*W 4.7T MRI image (T2*W value was 10.0 ms for VCAM-CLIO-Cy5.5 and 102.0 ms for IgG-CLIO-Cy5.5), indicating the present of VCAM-CLIO-Cy5.5 nanoparticles in the samples.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+nanoparticle+rodentia)]

Tsourkas et al. (15) performed in vivo intravital confocal microscopy in C57BL/6 mice subjected to subcutaneous injection of TNFα to the left ear to induce vascular inflammation within 24 h. After retino-orbital injection of either VCAM-CLIO-Cy5.5 or IgG-CLIO-Cy5.5 (165 μg Fe), both ears were imaged at 1, 6, and 24 h. VCAM-CLIO-Cy5.5 provided the greatest degree of cell-surface fluorescence intensity in the endothelium of the left ear at 6 h but not in the normal right ear. The fluorescence signal was lower at 24 h but was brighter than nonspecific IgG-CLIO-Cy5.5. The low fluorescence signal that came from IgG-CLIO-Cy5.5 is most likely because of nonspecific CLIO uptake at the site of inflammation at 24 h. No MR imaging or blocking experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+nanoparticle+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+nanoparticle+(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+nanoparticle+human)]

No publication is currently available.

## NIH Support

T32 CA79443, P50 CA86355

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
4 Wunderbaldinger P., Josephson L., Bremer C., Moore A., Weissleder R. (2002). Detection of lymph node metastases by contrast-enhanced MRI in an experimental model. Magn Reson Med.
5 Josephson L., Kircher M.F., Mahmood U., Tang Y., Weissleder R. (2002). Near-infrared fluorescent nanoparticles as combined MR/optical imaging probes. Bioconjug Chem.
6 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
7 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
8 Vanderslice P., Woodside D.G. (2006). Integrin antagonists as therapeutics for inflammatory diseases. Expert Opin Investig Drugs.
9 Bochner B.S., Luscinskas F.W., Gimbrone M.A., Newman W., Sterbinsky S.A., Derse-Anthony C.P., Klunk D., Schleimer R.P. (1991). Adhesion of human basophils, eosinophils, and neutrophils to interleukin 1-activated human vascular endothelial cells: contributions of endothelial cell adhesion molecules. J Exp Med.
10 Kume N., Cybulsky M.I., Gimbrone M.A. (1992). Lysophosphatidylcholine, a component of atherogenic lipoproteins, induces mononuclear leukocyte adhesion molecules in cultured human and rabbit arterial endothelial cells. J Clin Invest.
11 Leung K.H. (1999). Release of soluble ICAM-1 from human lung fibroblasts, aortic smooth muscle cells, dermal microvascular endothelial cells, bronchial epithelial cells, and keratinocytes. Biochem Biophys Res Commun.
12 Luscinskas F.W., Cybulsky M.I., Kiely J.M., Peckins C.S., Davis V.M., Gimbrone M.A. (1991). Cytokine-activated human endothelial monolayers support enhanced neutrophil transmigration via a mechanism involving both endothelial-leukocyte adhesion molecule-1 and intercellular adhesion molecule-1. J Immunol.
13 Nagel T., Resnick N., Atkinson W.J., Dewey C.F., Gimbrone M.A. (1994). Shear stress selectively upregulates intercellular adhesion molecule-1 expression in cultured human vascular endothelial cells. J Clin Invest.
14 Aikawa M., Libby P. (2004). The vulnerable atherosclerotic plaque: pathogenesis and therapeutic approach. Cardiovasc Pathol.
15 Tsourkas A., Shinde-Patil V.R., Kelly K.A., Patel P., Wolley A., Allport J.R., Weissleder R. (2005). In vivo imaging of activated endothelium using an anti-VCAM-1 magnetooptical probe. Bioconjug Chem.